# Microbubbles coated with antibody to intracellular adhesion molecule-1

Chemical name: | Microbubbles coated with antibody to intracellular adhesion molecule-1
Abbreviated name: | MB_ICAM-1_
Synonym:
Agent category: | Antibody
Target: | Intracellular adhesion molecule-1 (ICAM-1)
Target category: | Adhesion molecule
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=825682), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4557877) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3383) for more information about ICAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1)]

Ultrasound is widely used imaging modality (1) and is expanding its role in noninvasive molecular imaging with ligand-carrying microbubbles (2). Microbubbles are comprised of spherical cavities filled by a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles. Microbubbles are usually 2 to 8 μm in size. They provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They are also potentially used for drug and gene delivery (6).

Endothelial cells are important cells in inflammatory responses (7, 8). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1) and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their rolling along endothelial cell surfaces and subsequently adherence to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins and selectins. Chemokines are chemotactic to leukocytes to sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (9).

ICAM-1 is found on cell surface of endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (10-14). It binds to counter-receptors on the cell-surface of leukocytes. IL-1 and TNFα increase ICAM-1 and other cell adhesion molecule expression on the vascular endothelial cells, leading to leukocyte adhesion to the activated endothelium. Microbubbles targeted with antibody against ICAM-1 are being developed as a noninvasive agent for ICAM-1 expression in vascular endothelial cells of dysfunctional endothelium (15-18).

### Related Resource Links:

- Chapters in MICAD (ICAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=ICAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (ICAM-1 (http://www.ncbi.nlm.nih.gov/gene/3383))
- Articles in Online Mendelian Inheritance in Man (OMIM) (ICAM-1 (http://www.ncbi.nlm.nih.gov/omim/147840))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1%20and%20synthesis)]

For targeted microbubbles, Weller et al. (17) prepared biotinylated microbubbles by sonication of an aqueous dispersion of decafluorobutane gas, phosphatidylcholine, polyethyleneglycol-(PEG-) stearate, and phosphatidylethanolamine-biotin in a 2:1:1 ratio by weight. Microbubbles were combined with streptavidin, washed, and conjugated with biotinylated mouse monoclonal antibody against ICAM-1(MB_ICAM-1_) or isotype control monoclonal antibody (MB_iso_). Control lipid microbubbles (MB_c_) were also prepared. The microbubbles are about 3.4 ± 1.2 microns in diameter. An antibody to microbubble ratio was estimated to be 60,000 ± 5,000 by flow cytometry. Alternatively, the primary amino groups of antibody were covalently conjugated to the carboxylic groups on the microbubble shell, which has been activated with 1-ethyl-3-(3-dimethylaminopropyl) carbodiimide (15).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1%20and%20in%20vitro)]

Villanueva et al. (15) reported that MB_ICAM-1_ (1^_^10 x 10^8^/ml) perfused through the flow chamber coated with endothelial cells at a wall shear rate of 25 s^-1^. There was a significantly greater number of MB_ICAM-1_ attached to IL-1 activated endothelial cells (8.0 ± 3.5 microbubbles/cell) than to normal endothelial cells (0.21 ± 0.09 microbubbles/cell). The number of adherent MB_ICAM-1_ to activated endothelial cell decreased to 2.6 ± 0.3 and 0.8 ± 0.4 at 100 and 1000 s^-1^, respectively. The number of MB_ICAM-1_ adherent to normal endothelial cell was only 0.1 at 1000 s^-1^. MB_c_ and MB_iso_ attachment to both activated and normal endothelial cells were minimal (0.03-0.05) at 25 s^-1^ and there were no significant changes at higher wall shear rates.

Weller et al. (16, 17, 19) confirmed that microbubble shell antibody density and wall shear rate are critical parameters controlling microbubble targeted adhesion. Microbubble adhesion was significantly greater with greater anti-ICAM-1 antibody density of the microbubbles and greater ICAM-1 expression on the cell surface of the endothelial cells. On the other hand, microbubble adhesion to endothelial cells was inversely proportional to the wall shear rate. Therefore, accumulation and retention of MB_ICAM-1_ is possible under physiologic flow conditions and is strongly influenced by shear stress and surface density of the target receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1%20and%20rodentia)]

Weller et al. (16) performed ultrasound assessment of acute cardiac transplant rejection with 2.5x10^6^ MB_ICAM-1_ by triggered myocardial contrast echocardiography in rats. Cardiac ultrasound imaging of rejecting allograft transplants (10 ± 4 U, n = 8) showed that video intensity signal was significantly higher (P<0.01) than control isograft transplants (1 ± 4 U, n = 7) for MB_ICAM-1_. On the other hand, MB_c_ exhibited a minimal contrast in both the allograft and isograft transplants. Postmortem histology confirmed that the rejecting allograft transplants had a significantly higher ICAM-1 expression than the control isograft transplants.

Reinhardt et al. (18) performed ultrasound assessment of ICAM in experimental autoimmune encephalomyelitis (EAE) in rats by sensitive particle acoustic quantification (SPAQ), which allows qualification of microbubbles in high concentration and resolution in μm (20). EAE was induced by transferring myelin basic protein activated T-cells intravenously into rats. On day 4, the brain and spinal cord was excised 30 min after injection of MB_ICAM-1._ Registration of acoustic counts during the first scan of the brain and the spinal cord revealed a significant higher ICAM-1 expression in AT-EAE rats (P <0.001, n = 6) that received MB_ICAM-1_ (~10,000-15,000 acoustic counts) than AT-EAE rats (n = 4) that received unspecific MB_iso_ (~500 acoustic counts). In addition, only a marginal signal was detected in healthy controls (n = 4, ~500 acoustic counts) that received MB_ICAM-1_. Pretreatment of EAE rats with anti-ICAM-1 antibody or methylprednisolone (a therapeutic drug) before MB_ICAM-1_ injection decreased the acoustic counts by >75%. The whole brain scan of living anesthetized rats after injection of MB_ICAM-1_ confirmed the ex-vivo experiments that healthy control rats (n = 3) showed only a marginal acoustic signal, whereas EAE rats (n = 3) exhibited a strong acoustic signal similar to the ex-vivo EAE brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20ICAM-1%20and%20human)]

No publication is currently available.

## NIH Support

HL58865

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
8 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
9 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
10 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
11 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
12 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
13 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
14 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
15 Villanueva F.S., Jankowski R.J., Klibanov S., Pina M.L., Alber S.M., Watkins S.C., Brandenburger G.H., Wagner W.R. (1998). Microbubbles targeted to intercellular adhesion molecule-1 bind to activated coronary artery endothelial cells. Circulation.
16 Weller G.E., Lu E., Csikari M.M., Klibanov A.L., Fischer D., Wagner W.R., Villanueva F.S. (2003). Ultrasound imaging of acute cardiac transplant rejection with microbubbles targeted to intercellular adhesion molecule-1. Circulation.
17 Weller G.E., Villanueva F.S., Klibanov A.L., Wagner W.R. (2002). Modulating targeted adhesion of an ultrasound contrast agent to dysfunctional endothelium. Ann Biomed Eng.
18 Reinhardt M., Hauff P., Linker R.A., Briel A., Gold R., Rieckmann P., Becker G., Toyka K.V., Maurer M., Schirner M. (2005). Ultrasound derived imaging and quantification of cell adhesion molecules in experimental autoimmune encephalomyelitis (EAE) by Sensitive Particle Acoustic Quantification (SPAQ). Neuroimage.
19 Weller G.E., Villanueva F.S., Tom E.M., Wagner W.R. (2005). Targeted ultrasound contrast agents: in vitro assessment of endothelial dysfunction and multi-targeting to ICAM-1 and sialyl Lewisx. Biotechnol Bioeng.
20 Reinhardt M., Hauff P., Briel A., Uhlendorf V., Linker R.A., Maurer M., Schirner M. (2005). Sensitive particle acoustic quantification (SPAQ): a new ultrasound-based approach for the quantification of ultrasound contrast media in high concentrations. Invest Radiol.